# Cys-Asp-Cys-Arg-Gly-Asp-Cys-Phe-Cys/Cy5.5-Ferritin ^64^Cu-loaded nanocages

Chemical name: | Cys-Asp-Cys-Arg-Gly-Asp-Cys-Phe-Cys/Cy5.5-Ferritin ^64^Cu-loaded nanocages
Abbreviated name: | RGD4C/Cy5.5-Fn-^64^Cu nanocages
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography; optical, near-infrared (NIR) fluorescence
Source of signal: | ^64^Cu, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence (NIRF) imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Integrins are a family of heterodimeric, cell-surface glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (6). Integrins comprise an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class, affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (7-12). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of the α_v_β_3_ integrin is weak on resting endothelial cells and on most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (11, 13, 14). A tripeptide sequence comprising Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled cyclic RGD peptides have been introduced for tumor imaging and tumor angiogenesis (15).

Ferritin is composed of 24 subunits of heavy and light chains that self-assemble to form a cage-like nanoparticle (nanocage) at physiological pH (7.4) with internal and external diameters of 8 nm and 12 nm (16, 17), respectively. The outer surface of ferritin can be chemically or genetically modified with ligands, and the cavity of ferritin can capture metal ions with high affinity (18). Lin et al. (19) genetically grafted an α_v_β_3_-targeted peptide (RDCRGDCFC, RGD4C) onto heavy chain ferritin (RGD4C-Fn) and chemically coupled Cy5.5 onto heavy chain ferritin (Cy5.5-Fn). Hybridization of RGD4C-Fn and Cy5.5-Fn (1:1) in the presence of ^64^CuCl_2_ resulted in the formation of RGD4C/Cy5.5-ferritin ^64^Cu-loaded nanocages (RGD4C/Cy5.5-Fn-^64^Cu nanocages). RGD4C/Cy5.5-Fn-^64^Cu nanocages have been developed for positron emission tomography and NIRF multimodality imaging of tumor vasculature to study in vivo biodistribution of the tracer in tumor-bearing mice. RGD4C/Cy5.5-Fn-^64^Cu nanocages have been shown to have a high accumulation in the tumor vasculature and a predominant liver accumulation.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690), ferritin heavy chain (http://www.ncbi.nlm.nih.gov/gene/2495), ferritin light chain (http://www.ncbi.nlm.nih.gov/gene/2512))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+synthesis)]

Recombinant Fn and RGD4C-Fn were purified from transfected Escherichia coli cell lysates (19). Cy5.5-Fn was prepared by incubation of Cy5.5-NHS ester (100 nmol) with Fn (50 nmol) for 1 h at room temperature. Cy5.5-Fn was isolated with column chromatography. There was one Cy5.5 molecule per ferritin subunit. To prepare RGD4C/Cy5.5-Fn-^64^Cu nanocages, C-Fn and R-Fn (17 nmol each) were mixed at room temperature to form ferritin nanocages, which were then broken down to subunits by adjusting pH to 2. ^64^CuCl_2_ (222 MBq (6 mCi)) was added to the acidic solution, and the mixture was incubated for another 30 min. The pH was then adjusted back to pH 7.4 with 1 M NaOH, and the mixture was incubated for 30 min to form RGD4C/Cy5.5-Fn-^64^Cu nanocages. RGD4C/Cy5.5-Fn^-64^Cu nanocages were isolated with column chromatography. Approximately 60% of ^64^CuCl_2_ was loaded into RGD4C/Cy5.5-Fn-^64^Cu nanocages. Dialysis in phosphate-buffered saline and fetal bovine serum for 24 h showed that <10% of radioactivity was released from the nanocages under both conditions. The diameter of RGD4C-Fn was determined to be ~10 nm with dynamic light scattering analysis at pH 7.4 The diameter of RGD4C/Cy5.5-Fn^-64^Cu nanocages was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+in%20vitro)]

Lin et al. (19) performed competitive cell-binding assays using MDA-MB-435 human breast tumor cells, which express α_v_β_3_. RGD4C/Cy5.5-Fn, RGD4C-Fn, and RGD4C inhibited the binding of ^125^I-echistatin to MDA-MB-435 cells in a dose-dependent manner with 50% inhibition concentrations of 5.5 nM, 2.9 nM, and 24.4 nM, respectively. On the other hand, Cy5.5-Fn showed little inhibition of the binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+rodentia)]

Lin et al. (19) performed whole-body PET and NIRF imaging in nude mice (n = 3) bearing U87MG tumors after injection of 3.7 MBq (0.1 mCi) RGD4C/Cy5.5-Fn-^64^Cu nanocages. PET tumor accumulation of radioactivity levels were 6.4 ± 1.5% injected dose/gram (ID/g) at 1 h, 7.5 ± 0.7% ID/g at 4 h, 8.1 ± 0.1% ID/g at 24 h, and 7.5 ± 0.1% ID/g at 40 h. Preinjection of excess c(RGDyK) (0.5 mg, 30 min before the probe injection) resulted in tumor accumulation levels of 6.4 ± 2.3% ID/g at 1 h, 5.9 ± 1.8% ID/g at 4 h, 6.0 ± 1.3% ID/g at 24 h, and 4.4 ± 0.7% ID/g at 40 h. NIRF imaging showed a similar tumor accumulation profile with a marginal difference between blocking and non-blocking groups at 1 h after injection. Such a difference continued to increase, reaching a maximum at 40 h (442.3 ± 208.9 versus 1,373.9 ± 320.1 × 10^6^ photons cm−^2^s−^1^). The investigators suggested that the high tumor accumulation of RGD4C/Cy5.5-Fn-^64^Cu nanocages may be due to a combination of RGD-integrin interaction and the enhanced permeability and retention (EPR) effect. The latter would not be blocked by c(RGDyK) and subjected to washout. Ex vivo imaging at 40 h showed that the liver exhibited the highest radioactivity and NIRF signals, which were not blocked by c(RGDyK). On the other hand, both signals from the tumor were decreased by c(RGDyK). Immunostaining of the tumor sections showed that RGD4C/Cy5.5-Fn-^64^Cu nanocages primarily targeted the tumor vasculature through an RGD–integrin α_v_β_3_ interaction on the endothelial cells, with a good correlation between RGD signals and integrin signals. On the other hand, there was no correlation between RGD signals and integrin signals in the blocking group, suggesting primarily the EPR effect.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Gurfinkel M., Ke S., Wen X., Li C., Sevick-Muraca E.M. (2003). Near-infrared fluorescence optical imaging and tomography. Dis Markers.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
7 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
8 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
9 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
10 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
11 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
12 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
13 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
14 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
15 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
16 Maham A., Tang Z., Wu H., Wang J., Lin Y. (2009). Protein-based nanomedicine platforms for drug delivery. Small.
17 Uchida M., Kang S., Reichhardt C., Harlen K., Douglas T. (2010). The ferritin superfamily: Supramolecular templates for materials synthesis. Biochim Biophys Acta.
18 Uchida M., Flenniken M.L., Allen M., Willits D.A., Crowley B.E., Brumfield S., Willis A.F., Jackiw L., Jutila M., Young M.J., Douglas T. (2006). Targeting of cancer cells with ferrimagnetic ferritin cage nanoparticles. J Am Chem Soc.
19 Lin X., Xie J., Niu G., Zhang F., Gao H., Yang M., Quan Q., Aronova M.A., Zhang G., Lee S., Leapman R., Chen X. (2011). Chimeric ferritin nanocages for multiple function loading and multimodal imaging. Nano Lett.